# Humanized anti–type 1 insulin-like growth factor receptor monoclonal antibody conjugated to Alexa 680

Chemical name: | Humanized anti–type 1 insulin-like growth factor receptor monoclonal antibody conjugated to Alexa 680
Abbreviated name: | AVE1642-Alexa 680
Synonym:
Agent Category: | Antibody
Target: | Type 1 insulin-like growth factor receptor (IGF1R)
Target Category: | Receptor
Method of detection: | Near-infrared (NIR) fluorescence
Source of signal / contrast: | Alexa 680
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ave1642)]

Overexpression and activation of the type 1 insulin-like growth factor receptor (IGF1R), which mediates its activity through an associated tyrosine kinase, is believed to promote the progression and metastasis of several cancers (1-3). In addition, higher than normal or overexpression of the IGF1R itself, or any of its different constituent parts, is considered to indicate an aggressive or drug-resistant cancer phenotype with a poor prognosis for the patient (3). As a consequence, the IGF1R is a target of various agents, including monoclonal antibodies (mAbs) directed against it, that are under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=IGF1R) approved by the United States Food and Drug Administration for the treatment of cancers. Also, using xenograft tumor models, a downregulation in IGF1R expression has been shown to be accompanied by reduced tumor growth, suggesting that IGF1R levels can be used to monitor patient response to anti-cancer treatment(s) (4, 5).

The epidermal growth factor receptor (EGFR), which is known to be overexpressed in several cancers, is routinely quantified in a clinical setting using in situ hybridization or immunohistochemical techniques for biopsy samples, and the data obtained from these investigations are used to select patients who are most likely to benefit from an anti-EGFR therapy (6, 7). However, no such quantification is available for IGF1R expression, which has been quantified only in cultured cells using a humanized anti-IGF1R mAb (AVE1642) conjugated to cadmium telluride quantum dots (AVE1642 QD) (8). Zhang et al. developed and evaluated the use of Alexa 680 (a near-infrared fluorescent dye with a maxima at 705 nm) covalently linked to AVE1642 (AVE1642-Alexa 680) in a mouse model for the detection and imaging of xenograft tumors that express IGF1R (9). For comparison the investigators also evaluated the use of AVE1642 QD (discussed in a separate chapter of MICAD; www.micad.nih.gov) for the detection and imaging of the tumors expressing IGF1R (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+synthesis)]

The AVE1642 mAb was obtained from a commercial source, and its fluorescent labeling was performed with a commercially available Alexa 680 kit according to manufacturer instructions (9). The conjugate was purified with size-exclusion chromatography on a Superdex G200 column as described by Zhang et al. (9). The number of Alexa 680 molecules conjugated to each mAb molecule and the stability of the complex under in vitro or in vivo conditions were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+in+vitro)]

The receptor binding ability of AVE1642-Alexa 680 was investigated using MCF-7 cells, a breast cancer cell line that expresses high levels of IGF1R (9). The cells were exposed to AVE1642-Alexa 680, Alexa 680 alone (control), and an anti-CD20 antibody conjugated to Alexa 680 (negative control) for 1 h at 4°C in phosphate-buffered saline (PBS) containing 1% bovine serum albumin and 0.1% sodium azide. Binding of the fluorescent mAbs or the Alexa 680 alone was analyzed with fluorescence-assisted cell sorting (FACS). Only cells exposed to AVE1642-Alexa 680 were reported to bind to the MCF-7 cells.

In another study, mouse embryo fibroblast R cells (lacking the IGF1R gene) transfected with the IGF1R (R-/IGF1R cells) were shown with FACS analysis to bind AVE1642-Alexa 680 (9). Pretreatment of the R-/IGF1R cells with AVE1642 for 24 h was reported to eliminate the binding of AVE1642-Alexa 680 to the cells, indicating that the conjugated mAb bound specifically to the IGF1R.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+rodentia)]

Zhang et al. used athymic mice bearing xenograft tumors generated with either R-/IGF1R or MCF-7 cells to investigate the in vivo specificity of AVE1642-Alexa 680 (9). Mice bearing R-/IGF1R tumors were injected with 0.1 nmol conjugated mAb through the tail vein (control animals were injected with PBS alone), and whole-body imaging of the animals was performed at 2 h, 5 h, and 1, 2, 4, and 10 days after the treatment (the number of animals used per time point was not reported). After 1 day, Alexa 680–specific fluorescence was observed only in tumors of animals treated with AVE1642-Alexa 680, with the signal lasting for at least 4 days and diminishing by day 10. However the degree of reduction in signal was not reported by the investigators. No fluorescence was observed in the control animals or in any other organs or tissues of mice injected with the AVE1642 conjugate. Ex vivo imaging of the tumors, organs, and tissues confirmed that the fluorescent signal was present only at the tumor sites.

To confirm that the fluorescence observed in the tumor-bearing animals was only from the conjugated mAb, mice bearing MCF-7 tumors were injected with either AVE1642-Alexa 680 or the anti-CD20 antibody conjugated to Alexa 680 through the tail vein. The number of animals used per group was not specified (9). Whole-body imaging was performed on the animals after 2 days, and a fluorescent signal was observed only in tumors of mice injected with AVE1642-Alexa 680. Presence of the fluorescent signal at the tumor sites was confirmed with ex vivo imaging of the tumors.

In another study, mice bearing R-/IGF1R tumors were pretreated with 200 μg AVE1642 (injected intraperitoneally), and 2 days later the animals were injected with AVE1642-Alexa 680. Control animals were not pretreated with the anti-IGF1R mAb.The number of animals used per agent group was not provided (9). Exposure of IGF1R-positive tumors to AVE1642 was shown by Sachdev et al. to downregulate the number of receptors on the tumor cells (10), and this was reflected by the reduced fluorescence, compared with controls, observed with the tumors pre-exposed to AVE1642.

From these studies the investigators concluded that AVE1642-Alexa 680 could be used to detect and quantify IGF1R in rodents under in vivo conditions (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AVE+1642+Alexa+680+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 McCampbell A.S., Broaddus R.R., Loose D.S., Davies P.J. (2006). Overexpression of the insulin-like growth factor I receptor and activation of the AKT pathway in hyperplastic endometrium. Clin Cancer Res.
2 Yuen J.S., Akkaya E., Wang Y., Takiguchi M., Peak S., Sullivan M., Protheroe A.S., Macaulay V.M. (2009). Validation of the type 1 insulin-like growth factor receptor as a therapeutic target in renal cancer. Mol Cancer Ther.
3 Hewish M., Chau I., Cunningham D. (2009). Insulin-like growth factor 1 receptor targeted therapeutics: novel compounds and novel treatment strategies for cancer medicine. Recent Pat Anticancer Drug Discov.
4 Goetsch L., Gonzalez A., Leger O., Beck A., Pauwels P.J., Haeuw J.F., Corvaia N. (2005). A recombinant humanized anti-insulin-like growth factor receptor type I antibody (h7C10) enhances the antitumor activity of vinorelbine and anti-epidermal growth factor receptor therapy against human cancer xenografts. Int J Cancer.
5 Shang Y., Mao Y., Batson J., Scales S.J., Phillips G., Lackner M.R., Totpal K., Williams S., Yang J., Tang Z., Modrusan Z., Tan C., Liang W.C., Tsai S.P., Vanderbilt A., Kozuka K., Hoeflich K., Tien J., Ross S., Li C., Lee S.H., Song A., Wu Y., Stephan J.P., Ashkenazi A., Zha J. (2008). Antixenograft tumor activity of a humanized anti-insulin-like growth factor-I receptor monoclonal antibody is associated with decreased AKT activation and glucose uptake. Mol Cancer Ther.
6 Meche A., Cimpean A.M., Raica M. (2009). Immunohistochemical expression and significance of epidermal growth factor receptor (EGFR) in breast cancer. Rom J Morphol Embryol.
7 Martin V., Mazzucchelli L., Frattini M. (2009). An overview of the epidermal growth factor receptor fluorescence in situ hybridisation challenge in tumour pathology. J Clin Pathol.
8 Zhang H., Sachdev D., Wang C., Hubel A., Gaillard-Kelly M., Yee D. (2009). Detection and downregulation of type I IGF receptor expression by antibody-conjugated quantum dots in breast cancer cells. Breast Cancer Res Treat.
9 Zhang H., Zeng X., Li Q., Gaillard-Kelly M., Wagner C.R., Yee D. (2009). Fluorescent tumour imaging of type I IGF receptor in vivo: comparison of antibody-conjugated quantum dots and small-molecule fluorophore. Br J Cancer.
10 Sachdev D., Singh R., Fujita-Yamaguchi Y., Yee D. (2006). Down-regulation of insulin receptor by antibodies against the type I insulin-like growth factor receptor: implications for anti-insulin-like growth factor therapy in breast cancer. Cancer Res.